# Cross-linked iron oxide–C-AHA-AREPPTRTFAYWGK(FITC)

Chemical name: | Cross-linked iron oxide–C-AHA-AREPPTRTFAYWGK(FITC)
Abbreviated name: | CLIO-EPPT
Synonym:
Agent Category: | Iron oxide, peptide
Target: | Tumor antigen
Target Category: | Binding
Method of detection: | Magnetic resonance imaging (MRI), Optical (NIRF)
Source of signal: | Iron oxide, Cy5.5, FITC
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO%20EPPT)]

Early tumor detection is crucial for successful cancer therapy and can greatly improve a patient’s survival rate. Equally important is the in vivo assessment of the outcome of cancer therapy. However, developing effective methods to serve these purposes remains one of the most difficult challenges. It would be very useful to develop a method that can non-invasively detect tumors at an early stage and also can monitor tumor progression/regression during the course of therapy.

An agent that specifically targets tumors with the combination of high-resolution imaging modalities would allow one to extract anatomical, physiological, and molecular information from the field of interest. Magnetic resonance (MR) imaging provides high-resolution spatial images in small animals and in humans (1). Near-infrared fluorescence (NIRF) imaging has less interference from tissue than short-wavelength fluorescence and provides great signal-to-noise ratio in small animals. Therefore, the combination of MR and NIRF technologies into an agent that possesses a tumor-specific function would allow one to obtain comprehensive information about tumor location, environment, and status in small animals (2, 3).

Mucin-1 (MUC-1) is a transmembrane molecule that is expressed by most glandular epithelial cells. Underglycosylated mucin-1 antigen (uMUC-1) is one of the early hallmarks of tumorigenesis and is overexpressed and underglycosylated in almost all human epithelial cell adenocarcinomas and in non-epithelial cancer cell lines, as well as in hematological malignancies (3). MUC-1 is heavily glycosylated in normal tissues, whereas in neoplastic tissues MUC-1 is underglycosylated. The oligosaccharide chains of uMUC-1 are prematurely terminated by the addition of sialic acids, thus permitting the immune system to access the peptide core of this antigen and reveal epitopes. This feature makes it possible to design a probe that discriminates between the normal cells and adenocarcinoma cells. Therefore, uMUC-1 antigen becomes an excellent target for imaging that can be recognized by a probe that exhibits multiple imaging modalities.

A multimodal imaging probe featuring imaging properties (CLIO-Cy5.5, MR, and NIRF) and a short peptide (C-AHA-AREPPTRTFAYWGK(FITC), or EPPT) that specifically recognizes human uMUC-1 antigen was designed. CLIO-Cy5.5 is a multimodal agent that consists of a super-paramagnetic iron oxide nanoparticle (CLIO) and a NIR fluorochrome (Cy5.5). It serves as a contrast agent for MR imaging and at the same time provides a NIRF image. The EPPT peptide was derived from the third heavy-chain complementarity-determining region (CDR3 V_h_) of the antibody ASM2 raised against human epithelial cancer cells (4, 5).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO%20EPPT)]

The synthesis of CLIO-EPPT was described by Medarova et al. (2) and Moore et al (3). In brief, EPPT peptides were synthesized using solid-phase peptide synthesis via 9-fluorenylmethyloxycarbonyl (Fmoc) chemistry. A 6-aminohexanoic acid (AHA) served as a linker between the EPPT peptide and the terminal cysteine, which was utilized through a thiol group to conjugate the peptide with CLIO nanoparticles. Fluorescein isothiocyanate (FITC) was incorporated into the peptide through the side chain amino group on lysine. CLIO-NH_2_ nanoparticles (produced by mixing CLIO nanoparticles with dextran, followed by activation with epichlorohydrin and ammonia) (6, 7), were mixed with Cy5.5 solution and incubated at room temperature overnight. Purified Cy5.5-CLIO-NH_2_ was further activated by reacting with succinimidyl iodoacetate. The activated Cy5.5-CLIO-NH_2_ was then conjugated with the EPPT peptide through the thiol group of the terminal cysteine. The size of the nanoparticle was determined using laser light scattering to be 35.8 nm, with an average of 14 EPPT peptides and 5 Cy5.5 dyes per iron oxide particle.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO-EPPT%20AND%20in%20vitro)]

A variety of human uMUC-1–positive tumor cell lines from different organs were used to quantitate CLIO-EPPT binding ability (3). These cell lines include ZR75-1 (breast), BT-20 (breast), HT-29 (colon), CAPAN-2 (pancreas), LS174T (colon), and ChaGo-K-1 (lung). The control cell lines include an uMUC-1–negative U87 glioblastoma line and normal lines that are heavily glycosylated (MCF10A and embryonic kidney 293 cell line). The control cell lines displayed a significantly lower binding of ^125^I-labeled CLIO-EPPT compared with the adenocarcinoma cell lines. Similar results were obtained from flow cytometry analysis, although the staining intensities varied, possibly due to varying glycosylation of different cell lines.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO-EPPT%20AND%20Rodentia)]

MR and NIRF images of mice injected with bilateral uMUC-1–positive and uMUC-1–negative tumors were taken before and 24 h after the i.v. injection of CLIO-EPPT (3). Significant MR signal reduction was observed in some regions of uMUC-1–positive tumors (52%, 53%, and 43% decrease for LS174T, CAPAN-2, and ChaGo-K-1 tumors, respectively, versus a 13–18% decrease in the uMUC-1–negative control U87 tumors). NIRF images taken immediately after the MR scan showed high NIRF intensities from the uMUC-1–positive tumors (HT-29, LS174T, ChaGo-K-1, and CAPAN-2), whereas no significant signal was observed from the uMUC-1–negative control U87 tumor. The data from NIRF imaging showed that uMUC-1–positive tumors accumulated 3.4-fold more CLIO-EPPT than uMUC-1–negative tumors.

A preclinical orthotopic model of human pancreatic cancer was used to demonstrate the tumor-specific accumulation of CLIO-EPPT (2). The uMUC-1–positive human pancreatic adenocarcinoma cell line CAPAN-2 was surgically implanted into mice. CLIO-EPPT was injected intravenously into the mice 13 days after tumor implantation. MR images were taken before and 24 h after the administration of CLIO-EPPT. Both the reduction of T2 relaxation rates and the high NIRF signal at the tumor location indicated the accumulation of CLIO-EPPT on the tumor. Tumor progression/regression was monitored with CLIO-EPPT after chemotherapeutic treatment. MR imaging results showed that there was no change in tumor size of the treated mice, whereas the untreated mice had a three-fold size increase 21 days after the tumor implantation. Semi-quantitative analysis from NIRF imaging showed 2.8-fold size increases in untreated mice and no changes in treated mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO-EPPT%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No relevant publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO-EPPT%20AND%20%28primate%20NOT%20human%29)]

No relevant publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO-EPPT%20AND%20human)]

No relevant publication is currently available.

## References

1 Weissleder R. (2002). Scaling down imaging: molecular mapping of cancer in mice. Nat Rev Cancer.
2 Medarova Z, Pham W, Kim Y, Dai G, Moore A. (2006). In vivo imaging of tumor response to therapy using a dual-modality imaging strategy. Int J Cancer.
3 Moore A, Medarova Z, Potthast A, Dai G. (2004). In vivo targeting of underglycosylated MUC-1 tumor antigen using a multimodal imaging probe. Cancer Res.
4 Hussain R, Courtenay-Luck NS, Siligardi G. (1996). Structure-function correlation and biostability of antibody CDR-derived peptides as tumour imaging agents. Biomed Pept Proteins Nucleic Acids.
5 5. Sivolapenko, G.B., V. Douli, D. Pectasides, D. Skarlos, G. Sirmalis, R. Hussain, J. Cook, N.S. Courtenay-Luck, E. Merkouri, K. Konstantinides, and et al., Breast cancer imaging with radiolabelled peptide from complementarity-determining region of antitumour antibody. Lancet, 1995. 346(8991-8992):1662-1666.
6 Josephson L, Perez JM, Weissleder R. (2001). Magnetic Nanosensors for the Detection of Oligonucleotide Sequences. Angew Chem Int Ed Engl.
7 Josephson L, Tung CH, Moore A, Weissleder R. (1999). High-efficiency intracellular magnetic labeling with novel superparamagnetic-Tat peptide conjugates. Bioconjug Chem.